# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-anti-prostate-specific membrane antigen 3/A12 monoclonal antibody

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-anti-prostate-specific membrane antigen 3/A12 monoclonal antibody
Abbreviated name: | ^64^Cu-DOTA-3/A12
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | PET
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12)]

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (1, 2). It has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (2). PSMA was found to have N-acetyl α-linked acidic dipeptidase or glutamate carboxypeptidase II activity (3). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, and in the absorption of folate (4). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (2). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody (^111^In-labeled Capromomab pendetide (^111^In-CYT-356)) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (5). In addition, the antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (6, 7). Monoclonal antibody (mAb) 3/A12 was found to be reactive with purified PSMA; 3/A12 also showed a strong and specific binding to LNCaP human prostate cancer cells and PSMA-transfected cells in culture (8). ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-3/A12 mAb (^64^Cu-DOTA-3/A12) has been studied for use in positron emission tomography (PET) to image PSMA expression in nude mice bearing human cancer xenografts (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20AND%20synthesis)]

DOTA-3/A12 was incubated with ^64^CuCl_2_ for 40 min at 40°C (9). ^64^Cu-DOTA-3/A12 was purified with high-performance liquid chromatography. The radiochemical purity was 95% with a specific radioactivity of 67.3 MBq/nmol (1.8 mCi/nmol). ^64^Cu-DOTA-3/A12 was stable in saline buffer and mouse serum at 37°C for up to 24 h. The number of DOTA molecules per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20AND%20in%20vitro)]

The binding affinity of 3/A12 and DOTA-3/A12 for PSMA was determined with the use of PSMA-expressing C4-2 prostate cancer cells (9). In this assay, phycoerythrin-labeled ant-IgG was used as a secondary antibody for cytofluorometric analysis. The concentrations that reached a 50% saturation of PSMA sites were 10 nM for 3/A12 and 15 nM for DOTA-3/A12.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20and%20rodentia)]

Elsasser-Beile et al. (9) performed ex vivo biodistribution studies of ^64^Cu-DOTA-3/A12 (~0.15 nmol) in nude mice bearing PSMA-positive C4-2 tumor xenografts (n = 8 mice) or PSMA-negative DU 145 tumor (n = 7 mice) xenografts. The C4-2 tumor uptake was 35.1 ± 8.0% injected dose per gram (ID/g) at 48 h after injection. The tumor/muscle and tumor/blood ratios were 27 and 2, respectively. On the other hand, the radioactivity level in DU 145 tumors was 12.8 ± 2.7% ID/g. The organ with the highest accumulation was the liver (10% ID/g), followed by the kidneys (6% ID/g), heart (5% ID/g), colon (3% ID/g), and stomach (2% ID/g). The whole-body distribution of ^64^Cu-DOTA-3/A12 was also assessed with PET imaging at 3, 24, and 48 h after injection. The tumor/muscle ratios for the C4-2 tumors were 3.3, 7.8, and 9.6 at these time points, respectively. The C4-2 tumor exhibited a two-fold higher radioactivity than the DU 145 tumor at 24 h after injection. The highest radioactivity levels were visualized in the liver and the C4-2 tumor; the DU 145 tumors were barely visualized. Pretreatment with 5 nmol mAb 3/A12 3 h before ^64^Cu-DOTA-3/A12 injection in mice bearing the C4-2 tumors inhibited the radioactivity accumulation nearly to the background level of the DU 145 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=3/A12%20AND%20human)]

No publication is currently available.

## References

1 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
2 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
3 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
4 O'Keefe, D., D. Bachich, and W.D. Heston, Prostate specific membrane antigen. Prostate cancer, biology, genetics, and the new therapeutics., ed. L. Chung, W. Issacs, and J. Simons. 2001, New Jersey: Humana Press. 307-326.
5 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
6 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
7 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
8 Elsasser-Beile U., Wolf P., Gierschner D., Buhler P., Schultze-Seemann W., Wetterauer U. (2006). A new generation of monoclonal and recombinant antibodies against cell-adherent prostate specific membrane antigen for diagnostic and therapeutic targeting of prostate cancer. Prostate.
9 Elsasser-Beile U., Reischl G., Wiehr S., Buhler P., Wolf P., Alt K., Shively J., Judenhofer M.S., Machulla H.J., Pichler B.J. (2009). PET Imaging of Prostate Cancer Xenografts with a Highly Specific Antibody against the Prostate-Specific Membrane Antigen. J Nucl Med.